# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser
Abbreviated name: | ^64^Cu-DOTA-AE105, ^64^Cu-DOTA-D-Cha-F-s-r-Y-L-W-S
Synonym:
Agent category: | Peptide
Target: | Urokinase-type plasminogen activator receptor (uPAR)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=48146021), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=48146020) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=5329) for more information about uPAR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play an important role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degradation of the basement membrane and ECM (3). Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis (4-7).

Urokinase-type plasminogen activator (uPA) is a serine protease (8, 9). The uPA and uPA receptor (uPAR) system is responsible for tissue degradation after plasminogen activation to plasmin, which leads to a cascade of proteolysis or thrombolysis depending on the physiological conditions. uPA also directly activates MMPs, vascular endothelial growth factor, and human growth factor (10). Malignant tumors often express high levels of uPA and uPAR (11); therefore, the uPA/uPAR system is linked to vascular diseases and cancer. A synthetic peptide, Asp-cyclohexylalanine-Phe-D-Ser-D-Arg-Tyr-Leu-Trp-Ser (AE105), has been identified to have high affinity (dissociation constant (K_d_) = 0.4 nM) for human uPAR (12), and it has been labeled with ^64^Cu as ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-AE105 (^64^Cu-DOTA-AE105) for use in positron emission tomography (PET) imaging of uPAR expression in tumors (13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+synthesis)]

Li et al. (13) performed ^64^Cu labeling of AE105 through DOTA chelation. DOTA was activated by a five-fold molar excess of N-hydroxysuccinimide (pH 8) for 60 min. A mixture of AE105 and DOTA-OSSu in a molar ratio of 1:5 was incubated for 18 h at 4ºC. The DOTA-AE105 conjugate was purified with high-performance liquid chromatography (HPLC) with a 52% yield. The number of DOTA molecules per peptide was ~1. For radiolabeling, 20 μg DOTA-AE105 was added to 74 MBq (2 mCi) ^64^CuCl_2_ diluted in 0.1 M sodium acetate buffer (pH 6.5). The reaction mixture was incubated for 1 h at 50ºC. ^64^Cu-DOTA-AE105 was purified with HPLC (>98% radiochemical purity) with a radiolabeling yield of 80–90% (decay-corrected). ^64^Cu-DOTA-AE105_mut_, used as an inactive control, was prepared similarly. The specific activity of ^64^Cu-DOTA-AE105 and ^64^Cu-DOTA-AE105_mut_ was ~23 GBq/μmol (0.62 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+and+in+vitro)]

Li et al. (13) performed binding experiments with AE105, DOTA-AE105, and DOTA-AE105_mut_ with the use of a Biacore sensor chip immobilized with uPAR. The K_d_ value of AE105 was calculated to be 15 nM compared with the K_d_ value of 53 nM for DOTA-AE105; therefore, the binding affinity of DOTA-AE105 was 3.5-fold lower than the parent AE105. DOTA-AE105_mut_ binding was not detected up to 1,000 nM. AE105 and DOTA-AE105 inhibited the binding of pro-uPA to the immobilized uPAR with 50% inhibition concentration values of 16 and 130 nM, respectively. DOTA-AE105_mut_ exhibited little inhibition.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+rodentia)]

Li et al. (13) performed PET imaging studies at 1, 4.5, and 22 h after injection of ^64^Cu-DOTA-AE105 or ^64^Cu-DOTA-AE105_mut_ in mice (n = 3) bearing U87MG human glioblastomas (uPAR-positive) or MDA-MB-435 breast tumors (uPAR-negative). The initial accumulation of ^64^Cu-DOTA-AE105 in the U87MG tumors was 7.6% injected dose per gram (ID/g) at 1 h, and these levels increased to 10.8–10.9% ID/g at 4.5 and 22 h after injection. Pre-administration of AE105 (15 mg/kg) decreased tumor accumulation from 10.8% ID/g to 3.7% ID/g (P < 0.05) at 4.5 h after injection. On the other hand, tracer accumulation in the uPAR-negative tumors was low (<1% ID/g) at the three time points. The organs with the highest accumulation of ^64^Cu-DOTA-AE105 at 1 h after injection were the liver (10.9% ID/g) and kidneys (4.9% ID/g). The accumulation of ^64^Cu-DOTA-AE105_mut_ in U87MG tumors was only 1.7, 2.2, and 3.1% ID/g at 1, 4.5, and 22 h after injection, respectively. Immunohistochemical staining of frozen tumor sections confirmed the high expression of uPAR in the U87MG tumors but not in the MDA-MB-435 tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AE105+human)]

No publication is currently available.

## NIH Support

R01 CA119053, R21 CA121842, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Choong P.F. Nadesapillai A.P. Urokinase plasminogen activator system: a multifunctional role in tumor progression and metastasis Clin Orthop Relat Res 2003Suppl415 S46 58 14600592
9 Rabbani S.A., Mazar A.P. (2001). The role of the plasminogen activation system in angiogenesis and metastasis. Surg Oncol Clin N Am.
10 Folkman J., Shing Y. (1992). and , Angiogenesis.
11 Duffy M.J., Maguire T.M., McDermott E.W., O'Higgins N. (1999). Urokinase plasminogen activator: a prognostic marker in multiple types of cancer. J Surg Oncol.
12 Ploug M., Ostergaard S., Gardsvoll H., Kovalski K., Holst-Hansen C., Holm A., Ossowski L., Dano K. (2001). Peptide-derived antagonists of the urokinase receptor. affinity maturation by combinatorial chemistry, identification of functional epitopes, and inhibitory effect on cancer cell intravasation. Biochemistry.
13 Li Z.B., Niu G., Wang H., He L., Yang L., Ploug M., Chen X. (2008). Imaging of urokinase-type plasminogen activator receptor expression using a 64Cu-labeled linear peptide antagonist by microPET. Clin Cancer Res.